# S-[^11^C]Methyl-L-cysteine

Chemical name: | S-[^11^C]Methyl-L-cysteine
Abbreviated name: | [^11^C]MCYS
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter 1 (LAT1)
Target category: | Neutral amino acid uptake and protein synthesis
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissues (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, S-[^11^C]methyl-L-methionine ([^11^C]MET), and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in oncological imaging (1, 4, 5).

Some 20 amino acid transporter systems have been identified (1). Most amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system, a Na-dependent transporter system A, or a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their metabolic activities, including incorporation into proteins, which are higher than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells have been found to have overexpressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6) but are not approved by the United States Food and Drug Administration. These agents are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell except for leucine which is quantitatively incorporated into proteins. These natural amino acid images are based on amino acid transport and protein incorporation.

[^11^C]MET has been widely used in the detection of brain, head and neck, lung, and breast cancers as well as lymphomas (2) [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20human%20and%20neoplasm)]. [^11^C]MET can cross the blood–brain barrier, and while it is incorporated mainly into proteins, but [^11^C]MET is also incorporated into lipid, RNA, and DNA. [^11^C]MET PET imaging is more sensitive to radiotherapy compared to [^18^F]FDG and is useful for monitoring treatment of cancer. S-[^11^C]Methyl-L-cysteine ([^11^C]MCYS), an analog of [^11^C]MET, was evaluated as a PET tumor imaging agent (8).

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter 1 (http://www.ncbi.nlm.nih.gov/gene/8140), L-type amino acid transporter 2 (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), L-[^11^C]methionine (http://www.clinicaltrials.gov/ct2/results?term=11C+MET))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), L-[^11^C]methionine (http://google2.fda.gov/search?q=11C-methionine+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS%20and%20synthesis)]

A continuous flow procedure was automated for the synthesis of [^11^C]methyl iodide from [^11^C]CO_2_ and [^11^C]MCYS by ^11^C-meythylation of the desmethyl precursor L-cysteine with [^11^C]methyl iodide (8). The preparation was completed in 12 min after the end of bombardment, with a yield of >50% based on [^11^C]methyl iodide. The radiochemical purity of [^11^C]MCYS was >99%, with >90% enantiomeric purity. The specific activity of [^11^C]MCYS was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS%20and%20in%20vitro)]

Deng et al. (8) showed that [^11^C]MCYS accumulation in Hepa1-6 mouse hepatocellular carcinoma cells was reduced by 80% in the presence of 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (BCH, an L-type transporter inhibitor). The accumulation of [^11^C]MCYS was not affected by the presence of Na^+^ ions. On the other hand, no inhibition was observed in the presence of N-methyl-α-aminoisobutyric acid (an A-type transporter inhibitor) and L-alanine/serine/cysteine (System ASC). Specific transport of [^11^C]MCYS in Hepa1-6 cells was mediated mainly by System L and was independent of sodium ions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS%20and%20rodentia)]

Ex vivo tissue accumulation of [^11^C]MCYS was studied in normal mice at 5, 10, 20, 30, and 60 min after injection of 0.74–1.48 MBq (0.02–0.04 mCi) of the tracer (8). The tissue with the highest uptake at 5 min was the liver (1.97% injected dose (ID)/g)), followed by the blood (1.03% ID/g), stomach (0.99% ID/g), heart (0.94% ID/g), small intestine (0.92% ID/g), lung (0.91% ID/g), kidney (0.89% ID/g), brain (0.72% ID/g), and muscle (0.61% ID/g). All tissues showed moderate to rapid washout. At 30 min, the radioactivity levels were 0.86%, 0.21%, 0.44%, 0.40%, 0.46%, 0.38%, 0.32%, 0.18%, and 0.17% ID/g in the liver, blood, stomach, heart, small intestine, lung, kidney, brain, and muscle, respectively.

Deng et al. (8) performed whole-body PET imaging studies at 60 min after intravenous injection of 10 MBq (0.27 mCi) [^11^C]MCYS, [^18^F]FDG, or [^11^C]MET in female nude mice (n = 5/group) bearing Hepa1-6 tumors and turpentine-induced inflammation. The tumor accumulation of radioactivity was 4.58 ± 0.65% ID/g, 4.32 ± 0.47% ID/g, and 3.03 ± 0.79% ID/g for [^11^C]MCYS, [^18^F]FDG, and [^11^C]MET, respectively. The tumor/muscle ratios were 7.27, 5.08, and 4.26 for [^11^C]MCYS, [^18^F]FDG, and [^11^C]MET, respectively. Ex vivo tissue analysis at 30 min after injection showed that >99% of [^11^C]MCYS was not incorporated into proteins in the tumor, pancreas, brain, and blood . [^11^C]MCYS was >90% intact in these tissues. The inflammation accumulation of radioactivity was 1.02 ± 0.18% ID/g, 3.30 ± 0.23% ID/g, and 1.62 ± 0.68% ID/g for [^11^C]MCYS, [^18^F]FDG, and [^11^C]MET, respectively. The inflammation/muscle ratios were 1.62, 3.88, and 2.28 for [^11^C]MCYS, [^18^F]FDG, and [^11^C]MET, respectively. [^11^C]MCYS exhibited a higher tumor/muscle ratio and a lower inflammation/muscle ratio than did [^18^F]FDG and [^11^C]MET. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MCYS%20and%20human)]

[^11^C]MCYS and [^18^F]FDG PET brain imaging scans were performed in a 45-year-old male patient with grade IV glioma (8). [^18^F]FDG exhibited heterogeneous radioactivity in patches, whereas [^11^C]MCYS showed high radioactivity accumulation in the tumor lesion, which was confirmed with histopathological examination. Specific uptake was not determined.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Deng H., Tang X., Wang H., Tang G., Wen F., Shi X., Yi C., Wu K., Meng Q. (2011). S-11C-methyl-L-cysteine: a new amino acid PET tracer for cancer imaging. J Nucl Med.